# ^89^Zr-Labeled N-suc-desferrioxamine-conjugated anti-carbonic anhydrase IX chimeric monoclonal antibody cG250-F(ab’)_2_ fragments

Chemical name: | ^89^Zr-Labeled N-suc-desferrioxamine-conjugated anti-carbonic anhydrase IX chimeric monoclonal antibody cG250-F(ab’)_2_ fragments
Abbreviated name: | [^89^Zr]-cG250-F(ab')_2_
Synonym:
Agent Category: | Antibody
Target: | Carbonic anhydrase IX
Target Category: | Enzyme
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^89^Zr
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-carbonic%20anhydrase%20antibodies&cmd=DetailsSearch)]

Hypoxic tumors are often resistant to radio- and chemotherapy, have a high metastatic potential, and predict a poor outcome for the cancer patient (1). Although several methods (invasive and noninvasive) are available for the detection of hypoxia in tumors, including the use of radiolabeled small molecules, but these methods are not completely reliable because they either yield variable diagnoses, have functional limitations, show incomplete penetration of tumors, do not detect hypoxia in all tumor types, etc (1, 2). A common feature of most solid cancerous tumor types is the presence of hypoxic conditions (3) and the overexpression of carbonic anhydrase IX (CA IX), a transmembrane cell surface enzyme that is known to regulate the pH and adhesion of tumor cells (4). Therefore, as an alternative to the currently available agents used to detect hypoxic tumors, targeting the CA IX as a hypoxia biomarker is of great interest to investigators (1-3, 5). As an alternative to small molecules, the chimeric monoclonal antibody (cMab) cG250, directed against the CA IX, was developed, labeled with ^131^I, and evaluated as an immunotherapeutic agent for the detection and treatment of renal cell carcinoma (RCC) (6). This cMab was subsequently labeled with other nuclides (such as ^89^Zr, ^177^Lu, ^90^Y, etc.) and used in preclinical studies in rats (7) and in clinical trials for the radioimmunotherapy of RCC (6). However, only minor responses were observed in the clinical investigations and dose escalation studies are ongoing (6).

The ability of radiolabeled antibodies (Abs) used to detect or treat cancer is limited because these agents show only a peripheral penetration of solid tumors (due to large size, ~150 kDa) and leave many malignant cells untreated (8). In addition, Abs have a long blood circulation time and present a high radiation-absorbed dose to the bone marrow (9). It has been shown that, compared to intact Abs, the smaller monovalent Fab (~50kDa) or the divalent F(ab’)_2_ (~100 kDa) fragments derived from the parent Ab have a better tumor penetration and a shorter circulating half-life and are therefore likely to yield better results if used to detect or treat solid malignant tumors (8). With these observations in mind, a divalent F(ab’)_2_ fragment of cG250 was developed, labeled with ^131^I, and compared with the intact ^131^I-cG250 Ab for its pharmacokinetic behavior and tumor-targeting ability in mice and RCC patients (9). However, the investigators concluded that the intact Ab was superior to the divalent fragment for targeting the RCC tumors. Recently, the cG250-F(ab’)_2_ fragments were labeled with ^89^Zr (to produce [^89^Zr]-cG250-F(ab’)_2_) and evaluated for the visualization of tumor hypoxia in mice bearing SCCNij3 cell xenograft tumors (of human head and neck squamous cell carcinoma (http://www.skincancer.org/squamous-cell-carcinoma/) origin) with positron emission tomography (PET) (5).

### Other Sources of Information

Clinical trials (http://clinicaltrials.gov/ct2/results?term=Carbonic+anhydrase+IX+inhibitors) on carbonic anhydrase IX inhibitors

Human carbonic anhydrase IX in Entrez Gene (http://www.ncbi.nlm.nih.gov/gene/768) (Gene ID 768)

Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/169636419) of human carbonic anhydrase IX

Crystal structure of the human carbonic anhydrase IX catalytic domain (http://www.ncbi.nlm.nih.gov/Structure/mmdb/mmdbsrv.cgi?uid=76607)

Human carbonic anhydrase IX in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/nuccore?Db=omim&DbFrom=nuccore&Cmd=Link&LinkName=nuccore_omim&IdsFromResult=169636419) database

Hypoxia response in National Cancer Institute-Nature Pathways Interaction Database (http://pid.nci.nih.gov/search/pathway_landing.shtml?pathway_id=100145&pathway_name=hypoxia-inducible%20factor%20in%20the%20cardivascular%20system&source=BioCarta%20Imported&what=graphic&jpg=on&ppage=1)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=89Zr-labeled%20cG250-F%28ab%27%292%20synthesis&cmd=DetailsSearch)]

The production and labeling of the cG250-F(ab’)_2_ fragment with ^89^Zr (using N-suc-desferrioxamine as the chelating agent) was described in detail by Hoeben et al. (5). Labeling efficiency of the labeling reaction was reported to be 60% as determined with instant thin-layer chromatography (ITLC). Based on an ITLC analysis, the radiochemical purity of [^89^Zr]-cG250-F(ab’)_2_ was >95% with a specific activity of 0.41 MBq/μg (11.07 μCi/μg). Stability of the labeled Ab fragments was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=89Zr-labeled%20cG250-F%28ab%27%292%20in%20vitro&cmd=DetailsSearch)]

The immunoreactive fraction of [^89^Zr]-cG250-F(ab’)_2_ was determined to be 74% using SK-RC-52 tumor cells (derived from human metastatic RCC (10)) under in vitro conditions (5).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=89Zr-labeled%20cG250-F%28ab%27%292%20rodentia&cmd=DetailsSearch)]

In an ex vivo study to determine the correlation of spatial distribution of [^89^Zr]-cG250-F(ab’)_2_ to the microscopic distribution of tumor cells expressing CA IX, investigators injected mice bearing SCCNij3 cell xenograft tumors with the tracer; 4 h later, just before euthanization, the animals were injected with the pimonidazole stain (a hypoxia marker) and the Hoechst 33342 dye (a perfusion marker) (5). The tumors were removed from the animals, and an ex vivo autoradiographic analysis (for [^89^Zr]-cG250-F(ab’)_2_ uptake) and a histochemical analysis (for CA IX staining using an anti-CA IX Ab) of the tumors showed there was a significant (P < 0.0001) correlation (r = 0.57–0.74) between the CA IX staining and radioactivity uptake at both time points. A significant (P < 0.0001) correlation (r = 0.46–0.68) between pimonidazole staining and tracer uptake of the tumor was also reported at the two time points. In addition, a significant (P = 0.0067) correlation (r = 0.93) between the tumor maximum standardized uptake value and the tumor uptake determined ex vivo was reported. A similar correlation between CA IX and pimonidazole staining of tumor sections, respectively, and radioactivity accumulated in the tumor sections was also observed.

Mice bearing SCCNij3 cell xenograft tumors (n = 4 animals/time point) were injected intravenously with [^89^Zr]-cG250-F(ab’)_2_, and small-animal PET images were acquired at 4 h and 24 h post-injection (p.i.) (5). Tumors were clearly visible in the PET images at 4 h p.i., but the tumor image intensity was reduced by 24 h p.i. The percent injected dose per gram tissue (% ID/g) values for the tumor, blood, and muscles were ~3.75% ID/g, 4.50% ID/g, and 0.50% ID/g, respectively, at 4 h p.i. These values were reduced to ~1.60% ID/g, 0.20% ID/g, and 0.25% ID/g for the tumor, blood, and muscles, respectively, at 24 h p.i.

From these studies, the investigators concluded that [^89^Zr]-cG250-F(ab’)_2_ was a suitable tracer for the detection of head and neck xenograft tumors in a murine model. In addition, the accumulation of [^89^Zr]-cG250-F(ab’)_2_ in the tumor correlated well with the expression of CA IX in these tissue (5).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=89Zr-labeled%20cG250-F%28ab%27%292%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=89Zr-labeled%20cG250-F%28ab%27%292%20Non-Human%20Primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=89Zr-labeled%20cG250-F%28ab%27%292%20Human%20Studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Michalski, M.H. and X. Chen, Molecular imaging in cancer treatment. Eur J Nucl Med Mol Imaging. 2010
2 Mees G., Dierckx R., Vangestel C., Van de Wiele C. (2009). Molecular imaging of hypoxia with radiolabelled agents. Eur J Nucl Med Mol Imaging.
3 Carlin S., Khan N., Ku T., Longo V.A., Larson S.M., Smith-Jones P.M. (2010). Molecular targeting of carbonic anhydrase IX in mice with hypoxic HT29 colorectal tumor xenografts. PLoS One.
4 De Simone G., Supuran C.T. (2010). Carbonic anhydrase IX: Biochemical and crystallographic characterization of a novel antitumor target. Biochim Biophys Acta.
5 Hoeben B.A., Kaanders J.H., Franssen G.M., Troost E.G., Rijken P.F., Oosterwijk E., van Dongen G.A., Oyen W.J., Boerman O.C., Bussink J. (2010). PET of hypoxia with 89Zr-labeled cG250-F(ab')2 in head and neck tumors. J Nucl Med.
6 Stillebroer A.B., Oosterwijk E., Oyen W.J., Mulders P.F., Boerman O.C. (2007). Radiolabeled antibodies in renal cell carcinoma. Cancer Imaging.
7 Brouwers A., Verel I., Van Eerd J., Visser G., Steffens M., Oosterwijk E., Corstens F., Oyen W., Van Dongen G., Boerman O. (2004). PET radioimmunoscintigraphy of renal cell cancer using 89Zr-labeled cG250 monoclonal antibody in nude rats. Cancer Biother Radiopharm.
8 Schmidt M.M., Wittrup K.D. (2009). A modeling analysis of the effects of molecular size and binding affinity on tumor targeting. Mol Cancer Ther.
9 Brouwers A., Mulders P., Oosterwijk E., Buijs W., Corstens F., Boerman O., Oyen W. (2004). Pharmacokinetics and tumor targeting of 131I-labeled F(ab')2 fragments of the chimeric monoclonal antibody G250: preclinical and clinical pilot studies. Cancer Biother Radiopharm.
10 Gastl G., Ebert T., Finstad C.L., Sheinfeld J., Gomahr A., Aulitzky W., Bander N.H. (1996). Major histocompatibility complex class I and class II expression in renal cell carcinoma and modulation by interferon gamma. J Urol.